# ^111^In/^68^Ga-Labeled anti-epidermal growth factor receptor, native chemical ligation cyclized Affibody Z_HER2:342min_

Chemical name: | ^111^In/^68^Ga-Labeled anti-epidermal growth factor receptor, native chemical ligation cyclized Affibody Z_HER2:342min_
Abbreviated name: | [^111^In/^68^Ga]Z_HER2:342min_
Synonym:
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT) and gamma planar imaging; positron emission tomography (PET)
Source of signal / contrast: | ^111^In/^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342&cmd=DetailsSearch)]

The human epidermal growth factor receptor-2 (HER2, ErbB2) modulates its activity through a tyrosine kinase (TK) signaling pathway and is involved in the development of a variety of cancers (1, 2). Overexpression or amplification of the HER2 gene occurs in many cancer types (e.g., ~20% of breast cancer (BC)) and indicates a poor prognosis for the patient. Invasive methods such as biopsies, in conjunction with immunohistochemistry and in situ fluorescence hybridization, are often used to assess the HER2 status of the primary and metastasized neoplastic tumors; however, because of sampling bias and tumor heterogeneity, results obtained with these procedures are not completely reliable (2). In the clinic, ^18^F-labeled fluorodeoxyglucose is commonly used with positron emission tomography (PET) to detect and determine the tumor burden of a patient, but this imaging agent cannot distinguish between benign and malignant lesions, does not differentiate tumors that overexpress HER2 from those that have a low or no expression of the receptor, and often identifies inflammation as a false-positive neoplasm (1). Therefore, much effort has been devoted to produce and evaluate new imaging probes, such as radiolabeled anti-HER2 antibodies (3) and Affibodies (4), that can be used with single-photon emission computed tomography and PET to detect and diagnose cancers that overexpress HER2.

An Affibody molecule is a chain of 58 amino acids (~6.5 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained either via chemical synthesis or produced in bacteria with recombinant DNA technology (5). The Affibody scaffold consists of 3-helix peptide chains: helix chains 1 and 2 are each composed of thirteen randomized amino acids and contain the receptor-binding moieties of the Affibody (6), and the third helix chain functions as a stabilizer of the Affibody molecule (7). Affibody molecules have a high affinity and specificity of binding to the target, such as a receptor, and are considered to be extremely suitable for the noninvasive imaging of solid tumors (8). The radionuclide-labeled Affibody Z_HER2:342_ (and its derivatives), directed against the HER2 (Z_HER2:342_K_d_ = 22 pM for HER2), has been used successfully with molecular imaging techniques to screen for BC patients who can probably benefit most from treatment with trastuzumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=492dbdb2-077e-4064-bff3-372d6af0a7a2) (a monoclonal antibody that targets HER2) or lapatinib (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=63319b01-cad6-4d0a-c39b-938fa951a808) (a small molecule drug that inhibits the TK activity of the HER2 signaling pathway) (8, 9).

To further improve the imaging properties of radiolabeled Affibodies, it has been hypothesized that reducing the size of the molecule to a 2-helix structure will probably facilitate rapid clearance of the tracer from circulation, allow high penetration into solid tumors, ameliorate the uptake of label in non-targeted organs (such as the liver and lungs), and generate increased tumor/background ratios compared with the 3-helix molecule (10). To test this hypothesis, the third (stabilizing) helix chain was removed from the Z_HER2:342_ molecule; it was determined that the new 2-helix Affibody (MUT-DS; ~4.6 kDa) had a binding affinity of 5 nM for HER2 (10). In another study, ^68^Ga-labeled MUT-DS ([^68^Ga]-DOTA-MUT-DS) was evaluated for the detection of human ovarian carcinoma SKOV3 cell xenograft tumors, which overexpress HER2, in nude mice (11). Although the radioactivity from [^68^Ga]-DOTA-MUT-DS was rapidly cleared from circulation and had a high binding specificity for the tumors, the uptake of label in the neoplastic lesions was considerably lower (4.12 ± 0.83% of injected dose per gram tissue (ID/g) at 2 h postinjection (p.i.)) (11) than the accumulation with [^68^Ga]-ABY-002, another ^68^Ga-labeled HER2-binding 3-helix Affibody (12.4 ± 3.8% at 2 h p.i.) (12). This indicated that there was no particular advantage in using a smaller Affibody compared with the larger parent 3-helix molecule to detect tumors that overexpress HER2. The comparison between the two Affibody types was considered to be inaccurate because the data obtained with the two labeled Affibodies were generated in two separate and independent studies (6). In addition, the two SKOV3 cell subclones used to grow the tumors in mice in the two studies may not have produced identical lesions in the animals, and the same amounts of HER2 may not have been expressed in the neoplasms (6). Therefore, to ascertain the similarities or dissimilarities between MUT-DS and ABY-002 Affibodies, it was necessary to investigate the biological characteristics of the 2-helix and 3-helix Affibodies simultaneously using identical handling techniques and by performing similar in vitro and in vivo studies with the two Affibodies (6).

The receptor targeting and biodistribution characteristics of ^111^In-labeled MUT-DS (denoted as [^111^In]PEP09239) and ^111^In-labeled ABY-002 ([^111^In]ABY-002) were investigated by Rosik et al. in a side-by-side study with mice bearing xenograft tumors (6). It was observed that although the accumulation of label from [^111^In]ABY-002 in the tumors was higher than with [^111^In]PEP09239, the tumor/blood ratio was higher with the latter tracer. This indicated that both Affibody types are suitable for the imaging of tumors that expressed HER2. However, these probes can be easily degraded by circulating exoproteases because they are unprotected at the terminals, and, due to the presence of disulfide bonds in their structures, only a limited number of methods can be used to radiolabel either Affibody (7). In a continuing effort to develop a smaller 2-helix scaffold, it was shown that a native chemical ligation technique can be used to produce such a molecule (denoted as Z_min_) from the parental 2-helix Affibody (13). The characteristics of Z_min_ and the advantages of generating a molecular imaging probe based on the Z_min_ platform are discussed elsewhere (13). Hence, a backbone-cyclized version of the HER2-binding Z_HER2:342_ Affibody molecule, designated Z_HER2:342min_, was generated with the native chemical ligation technique and evaluated for its thermal stability, affinity, and selectivity for HER2 (7). Subsequently a DOTA-Z_HER2:342min_ conjugate was prepared for labeling with ^111^In and ^68^Ga, and the tumor-targeting and biodistribution characteristics of [^111^In]Z_HER2:342min_ and [^68^Ga]Z_HER2:342min_ were compared with those of [^111^In]PEP09239 and [^68^Ga]PEP09239 (7).

### Related Resource Links

Anti-HER2 Affibodies in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-HER2+affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=HER2) related to HER2

Other EGFR-imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/books?cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log$=booksrch&bname=micad)

EGFR (human) ligands in PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch)

Human EGFR in Online Mendelian Inheritance in Man database (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR))

Information on human EGFR gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein) (Gene ID: 1956)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding human EGFR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342min%20synthesis&cmd=DetailsSearch)]

The production, purification, and identification of Z_HER2:342min_ and PEP09239 have been described by Honarvar et al. (7). DOTA was conjugated to the third cysteine residue of each Affibody, and the conjugation was confirmed with electrospray ionization-mass spectroscopy. The DOTA-conjugated Affibodies were then radiolabeled with ^111^In and ^68^Ga as described elsewhere (7). The radiochemical yields (RCY) of [^111^In]Z_HER2:342min_ and [^111^In]PEP09239 were reported to be 98.75 ± 3.4% and 99.7 ± 0.0%, respectively, and the specific activities (SA) of both labeled Affibodies were ~3.9 MBq/μmol (105.4 μCi/μmol). The radiochemical purity (RCP) of [^111^In]Z_HER2:342min_ was 98.9 ± 0.1%; the RCP of [^111^In]PEP09239 was not reported. The RCYs of [^68^Ga]Z_HER2:342min_ and [^68^Ga]PEP09239 were 92.2 ± 1.9% and 97.1 ± 0.3%, respectively, with SAs of 9.6 GBq/μmol (0.259 Ci/μmol) and 3.9 GBq/μmol (0.105 Ci/μmol), respectively. The RCP of [^68^Ga]Z_HER2:342min_ was 99.2 ± 0.3%; the RCP of [^68^Ga]PEP09239 was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342min%20In%20Vitro%20Studies&cmd=DetailsSearch)]

The helicity of cyclic DOTA-Z_HER2:342min_ was investigated with circular dichroism analysis (7). The DOTA-conjugated Affibody was determined to have a minima between 208 nm and 220 nm and a maxima between 194 nm and 196 nm, indicating that the cyclic Affibody conjugate had a α-helical structure.

The DOTA-Z_HER2:342min_ conjugate was reported to have a high affinity for HER2 (K_d_ = 18 nM) as determined with surface plasmon resonance analysis (7). However, the K_d_ value obtained with the 2-helix Affibody conjugate was ~1,000-fold lower than the K_d_ value for the 3-helix parent Affibody molecule. Similar observations have been reported with other 2-helix Affibodies that target HER2 (7).

Both [^111^In]Z_HER2:342min_ and [^68^Ga]Z_HER2:342min_ were reported to maintain high stability (RCPs of 98.3 ± 0.3% and 98.3 ± 0.4%, respectively) when exposed to 500-fold excess ethylenediamine tetraacetic acid (7).

The in vitro binding characteristics of [^111^In]Z_HER2:342min_ and [^68^Ga]Z_HER2:342min_ were investigated using SKOV3 cells (high expression of HER2) and compared with those of [^111^In]PEP09239 and [^68^Ga]PEP09239 (7). All four radiolabeled Affibodies were shown to maintain their HER2 binding characteristics even after the labeling reaction. An analysis of the affinity titration curves obtained with the different tracers showed that the binding of the radiolabeled Affibodies to HER2 on the SKOV3 cells was mediated through two populations of the receptor as shown in Table 1 (7). Each radiolabeled Affibody was observed to exhibit a strong (in the pmol to nmol range) and a weak interaction (>10 nmol to >400 nmol range) with HER2. In general, the ^111^In-labeled Affibodies exhibited a higher affinity for HER2 compared with the ^68^Ga-labeled molecules (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342min%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]Z_HER2:342min_ and [^68^Ga]Z_HER2:342min_ was compared with that of [^111^In]PEP09239 and [^68^Ga]PEP09239 in BALB/c nu/nu mice bearing SKOV3 cell tumors (7). For the Z_HER2:342min_ Affibodies, the animals (n = 4 mice/radiolabeled Affibody per time point) were injected with a mixture of the tracers containing 10 kBq (0.27 μCi) [^111^In]Z_HER2:342min_ and 380 kBq (10.27 μCi) [^68^Ga]Z_HER2:342min_ (dose adjusted to ~28.5 nmol/animal with nonradioactive Z_HER2:342min_) through the tail vein, and the rodents were euthanized at 1 h p.i. and 2 h p.i. The amount of radioactivity accumulated in the various organs of interest was determined; results obtained from this study were presented as % ID/g (Table 2; only the data at 1 h p.i. are presented). In general, both radiolabeled Affibodies showed a similar biodistribution pattern in the animals, but the uptake of radioactivity from [^68^Ga]Z_HER2:342min_ in the lungs was ~5-fold higher than with [^111^In]Z_HER2:342min_. With [^111^In]Z_HER2:342min_, the uptake of radioactivity was significantly higher (P < 0.05) in the liver than with [^68^Ga]Z_HER2:342min_. The accumulation of radioactivity in the tumor was ~1.2-fold higher (P < 0.05) with [^111^In]Z_HER2:342min_ than with [^68^Ga]Z_HER2:342min_. Both radioconjugates exhibited renal excretion and showed tubular reabsorption in the kidneys (the uptake of label in these organs was >150% ID/g with both tracers). The tumor/blood, tumor/muscle, tumor/lung, and tumor/bone ratios were significantly higher with [^111^In]Z_HER2:342min_ than with [^68^Ga]Z_HER2:342min_ (for details, see Honarvar et al. (7)).

The tumor-targeting and HER2-binding specificity of [^111^In]Z_HER2:342min_ and [^68^Ga]Z_HER2:342min_ were established by determining the uptake of radioactivity from these labeled Affibodies in the tumors of mice (n = 4 animals/radiolabeled Affibody) preinjected (subcutaneously) with excess (3,800 nmol) nonradioactive Z_HER2:342min_ (7). A significantly reduced uptake (P < 0.05) of radioactivity was evident in the tumors with both radiolabeled Affibodies. This indicated that both [^111^In]Z_HER2:342min_ and [^68^Ga]Z_HER2:342min_ had a high binding specificity for HER2.

For comparison purposes, the studies described above were also performed with [^111^In]PEP09239 and [^68^Ga]PEP09239 in the same batch of BALB/c nu/nu mice bearing SKOV3 cell tumors (n = 4 animals/labeled Affibody) (7). Results obtained from these studies are presented in Table 2. A significantly higher (P < 0.05) uptake of radioactivity was observed in the tumors with [^111^In]PEP09239 (12 ± 4% ID/g) and [^68^Ga]PEP09239 (10.0 ± 3.2% ID/g) than with [^111^In]Z_HER2:342min_ (2.9 ± 0.7% ID/g) and [^68^Ga]Z_HER2:342min_ (2.4 ± 0.5% ID/g). The higher uptake of label observed with the PEP09239 tracers was attributed to the stronger affinity of these 2-helix Affibodies for HER2 compared with the affinities of the radiolabeled Z_HER2:342min_ homologs (7). In general, the accumulation of radioactivity with [^111^In]PEP09239 and [^68^Ga]PEP09239 in the various non-targeted organs was significantly lower (P < 0.05) than that observed with [^111^In]Z_HER2:342min_ and [^68^Ga]Z_HER2:342min_.

From these studies, the investigators concluded that the Z_HER2:342min_ tracers can target tumors that express HER2 in rodents (7). However, these tracers are probably not suitable for the detection of cancerous lesions because high levels of radioactivity from these radiolabeled Affibodies accumulate in the lungs, liver, and spleen, and the signal generated from the organs will mask the detection of any cancers that are metastasized to the organs or the surrounding tissues (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342min%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342min%20Non-Human%20Primates&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=ZHER2%3A342min%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Kramer-Marek G., Bernardo M., Kiesewetter D.O., Bagci U., Kuban M., Omer A., Zielinski R., Seidel J., Choyke P., Capala J. (2012). PET of HER2-Positive Pulmonary Metastases with 18F-ZHER2:342 Affibody in a Murine Model of Breast Cancer: Comparison with 18F-FDG. J Nucl Med.
2 Kramer-Marek G., Gijsen M., Kiesewetter D.O., Bennett R., Roxanis I., Zielinski R., Kong A., Capala J. (2012). Potential of PET to predict the response to trastuzumab treatment in an ErbB2-positive human xenograft tumor model. J Nucl Med.
3 Carlsson J. (2012). Potential for clinical radionuclide-based imaging and therapy of common cancers expressing EGFR-family receptors. Tumour Biol.
4 Wallberg H., Orlova A., Altai M., Hosseinimehr S.J., Widstrom C., Malmberg J., Stahl S., Tolmachev V. (2011). Molecular design and optimization of 99mTc-labeled recombinant affibody molecules improves their biodistribution and imaging properties. J Nucl Med.
5 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
6 Rosik D., Orlova A., Malmberg J., Altai M., Varasteh Z., Sandstrom M., Karlstrom A.E., Tolmachev V. (2012). Direct comparison of 111In-labelled two-helix and three-helix Affibody molecules for in vivo molecular imaging. Eur J Nucl Med Mol Imaging.
7 Honarvar H., Jokilaakso N., Andersson K., Malmberg J., Rosik D., Orlova A., Karlstrom A.E., Tolmachev V., Jarver P. (2013). Evaluation of backbone-cyclized HER2-binding 2-helix Affibody molecule for In Vivo molecular imaging. Nucl Med Biol.
8 Ahlgren S., Tolmachev V. (2010). Radionuclide molecular imaging using Affibody molecules. Curr Pharm Biotechnol.
9 Baum R.P., Prasad V., Muller D., Schuchardt C., Orlova A., Wennborg A., Tolmachev V., Feldwisch J. (2010). Molecular imaging of HER2-expressing malignant tumors in breast cancer patients using synthetic 111In- or 68Ga-labeled affibody molecules. J Nucl Med.
10 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
11 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.
12 Tolmachev V., Velikyan I., Sandstrom M., Orlova A. (2010). A HER2-binding Affibody molecule labelled with 68Ga for PET imaging: direct in vivo comparison with the 111In-labelled analogue. Eur J Nucl Med Mol Imaging.
13 Jarver P., Mikaelsson C., Karlstrom A.E. (2011). Chemical synthesis and evaluation of a backbone-cyclized minimized 2-helix Z-domain. J Pept Sci.

Table 1: Dissociation constants at equilibrium (K_d_) for binding of [^111^In]-Z_HER2:342min_, [^68^Ga]-Z_HER2:342min_, [^111^In]PEP09239, and [^68^Ga]PEP09239 to SKOV3 cells expressing HER2.

Radiolabeled conjugate | K _ d1 _ (nM) | K _ d2 _ (nM)
[ ^ 111 ^ In]-Z _ HER2:342min _ | 1.1 | 107
[ ^ 68 ^ Ga]-Z _ HER2:342min _ | 7.31 | 429
[ ^ 111 ^ In]PEP09239 | 0.32 | 64.1
[ ^ 68 ^ Ga]PEP09239 | 0.93 | 15.2

For complete data, see Honarvar et al. (7).

Table 2: Biodistribution of radioactivity from [^111^In]-Z_HER2:342min_, [^68^Ga]-Z_HER2:342min_, [^111^In]PEP09239, and [^68^Ga]PEP09239 in normal BALB/c nu/nu mice bearing SKOV3 cell xenograft tumors at 1 h p.i.

Organ | [ ^ 111 ^ In]-Z _ HER2:342min _ | [ ^ 111 ^ In]PEP09239 | [ ^ 68 ^ Ga]-Z _ HER2:342min _ | [ ^ 68 ^ Ga]PEP09239
Organ | Uptake of radioactivity (% ID/g)
Blood | 0.63 ± 0.05 | 0.5 ± 0.2 | 0.75 ± 0.05c (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0015) | 0.59 ± 0.20d (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0020)
Lung | 4.9 ± 3.2b (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0010) | 0.7 ± 0.2 | 23 ± 16a (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0005) | 1.0 ± 0.2d (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0020)
Liver | 9.8 ± 0.6b (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0010) | 1.8 ± 0.4 | 8.1 ± 1.0a (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0005)^,^c (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0015) | 2.4 ± 0.6d (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0020)
Kidney | 179 ± 14b (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0010) | 289 ± 44 | 158 ± 13a (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0005)^,^c (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0015) | 280 ± 39
Muscle | 0.17 ± 0.05 | 0.15 ± 0.04 | 0.18 ± 0.05 | 0.16 ± 0.02
Tumor | 2.9 ± 0.7b (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0010) | 12 ± 4 | 2.4 ± 0.5a (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0005)^,^c (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0015) | 10.0 ± 3.2d (http://www.sciencedirect.com/science/article/pii/S0969805112003204#tf0020)

a. P < 0.05 between [^68^Ga]--Z_HER2:342min_ and [^68^Ga]PEP09239.

b. P < 0.05 between [^111^In]-Z_HER2:342min_ and [^111^In]PEP09239.

c. P < 0.05 between [^68^Ga]-Z_HER2:342min_ and [^111^In]-Z_HER2:342min_.

d. P < 0.05 between [^68^Ga]PEP09239 and [^111^In]PEP09239.

For complete data, see Honarvar et al. (7).